# 4-[^18^F]Fluoro-2-D-methyl-3-mercaptopropanoyl-L-proline

Chemical name: | 4-[^18^F]Fluoro-2-D-methyl-3-mercaptopropanoyl-L-proline
Abbreviated name: | [^18^F]FCAP
Synonym: | 4-cis-[^18^F]-Fluorocaptopril
Agent Category: | Compound
Target: | Angiotensin-converting enzyme (ACE)
Target Category: | Inhibition of ACE
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluorocaptopril%5BAll%20Fields%5D)]

The renin–angiotensin system (RAS) plays a very important role in blood pressure regulation (1-4) in humans. Renin is an enzyme produced in the kidneys and it cleaves circulating angiotensinogen (a protein produced in the liver) to yield angiotensin I, an inactive decapeptide. The angiotensin-converting enzyme (ACE), found primarily in the lung, converts angiotensin I to angiotensin II, an active vasoconstrictor octapeptide. Angiotensin II also stimulates the production of aldosterone from the adrenal glands that promotes sodium and water retention. ACE is also responsible for inactivating bradykinin, a vasodilator (5). RAS and angiotensin II also play a role in interstitial fibrosis, cardiac remodeling and fibrosis, and heart failure (6, 7). It has also been shown that RAS operates in the heart, and the upregulation of this system is related to heart failure (8-10). Inhibition of ACE in patients with heart failure has often resulted in a favorable outcome for the patient (11). In this regard, captopril (2-D-methyl-3-mercaptopropanoyl-L-proline) was developed as an orally active ACE inhibitor and is considered an important drug for the treatment of hypertension. Subsequently, [^18^F]fluorocaptopril ([^18^F]FCAP) was developed for use with PET (12) to understand the in vivo dynamics of ACE activity.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluorocaptopril%20synthesis)]

[^18^F]FCAP was synthesized by Hwang et al. (12) as described here briefly. Diisopropylethyl amine was added to 4-trans-hydroxy-L-proline methyl ester hydrochloride suspended in methylene chloride, and the mixture was allowed to cool to 0^o^C. Then (R)-3-(acetylthio)-2-methylpropanoyl chloride was added to the cold mixture, and the reaction was allowed to warm to room temperature and stirred for 16 h. The reaction was quenched with sodium bicarbonate and the organic phase was dried over magnesium sulfate after washing with saturated sodium bicarbonate, 1 M hydrochloric acid, and saturated sodium chloride. The organic solvent was removed to obtain the crude product, which was then recrystallized from diethyl ether as a white solid. This solid (5 mg) was then dissolved in methylene chloride, cooled to 0^o^C, and combined with freshly distilled pyridine with triflic anhydride. The mixture was stirred for 15 min at 0^o^C, and the resulting clear, yellow, reaction mixture was transferred to a silica gel column for purification of the triflate analog by flash chromatography. A clear, oily, pure triflate (5 mg) was obtained.

The reference compound, nonradioactive cis-fluorocaptopril (FCAP), was prepared by Hwang et al. (12) by mixing the triflate analog of captopril with tetra-n-butylammonium fluoride followed by preparative high-performance liquid chromatography (HPLC) to obtain the pure standard material.To prepare [^18^F]FCAP, the triflate was solubilized in anhydrous acetonitrile (MeCN) and potassium ^18^F-labeled fluoride was added to it. The mixture was stirred for 5 min at room temperature. A short silica gel column was used to remove excess ^18^F-labeled fluoride and the reaction product was eluted with MeCN. Then 2 N NaOH (degassed with helium) was added to it. The mixture was acidified with concentrated HCl and diluted for purification by HPLC. After purification, the [^18^F]FCAP solution was adjusted to pH 6 with NaOH, filtered through a 0.22-micron filter, and used for animal studies. For human studies, the column was conditioned with ethanol followed by water for injection, and finally equilibrated with 10% ethanol (prepared in water for injection). The final purified preparation was tested for sterility and pyrogenicity.

The synthesis took 1 h and the purified product had a specific activity of >300 Ci/mmol with an average yield of 12% at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=in%20vitro%20testing%20of%20Fluorocaptopril)]

[^3^H]Captopril ([^3^H]CAP) binding has been studied in vitro in membranes of various rat tissues (13). The binding to these membranes was saturable and reversible with a K_D_ of 2.4 nM. In this study, Strittmatter et al. observed that [^3^H]CAP and ACE were distributed in parallel in the various tissues and the regions of the brain. The highest binding was observed in the coratoid plexus, lung, and corpus striatum, which strongly indicates that captopril selectively bound to ACE.

Other investigators have also studied the distribution of ACE in various animal tissues using radioactively labeled captopril, and the radiation was primarily detected in the kidney, lungs, and pituitary (14, 15). Radiation levels were shown to vary in different tissues, including the arteries, aorta, and adrenal medulla, depending on renin activity (16).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

[^18^F]FCAP biodistribution studies were performed in female Sprague-Dawley rats (12). The animals were killed 0.5, 1, 2, and 4 h after administration of [^18^F]FCAP. Blood, lungs, liver, spleen, kidney, heart, brain, bone, adrenal gland, aorta, and abdominal muscles were removed weighed, and incorporated radioactivity was measured. Maximum uptake was noted in the lungs, kidneys, and aorta. These organs are also known to have high concentrations of ACE.

In a titration study by the same investigators (12), the animals were co-injected with [^18^F]FCAP and differing amounts of unlabeled FCAP. The animals were killed 2 h postinjection. Blood, lungs, spleen, kidneys, heart, and aorta were removed form the animals and weighed, and incorporated radioactivity was measured. Compared to controls, low concentrations of unlabeled FCAP reduced the radioactivity by one half in the kidney, lung, and spleen. However, a much higher concentration of unlabeled FCAP was necessary to reduce the uptake in the aorta. This suggested that the uptake of [^18^F]FCAP binding with the ACE of this animal was saturable.

In a displacement study (12), the animals were first injected with [^18^F]FCAP, and 30 min later unlabeled FCAP was administered. The control animals received only [^18^F]FCAP. The animals were killed 1, 2, and 4 h after administration of [^18^F]FCAP. The control animals were killed 30 min after [^18^F]FCAP administration. The aorta, heart, lung, kidneys, and blood were removed from the animals and weighed, and incorporated radioactivity was measured. The displacement study demonstrated, in general, that tracer efflux from the various organs was very fast, which indicates that the binding of [^18^F]FCAP to ACE was reversible.

### Other Non-Primate Mammals: Dogs

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Markham et al. (17) developed a model in dogs to measure [^18^F]FCAP kinetics with pulmonary ACE by positron emission tomography (PET). In a companion publication (18), it was shown that a reduction in pulmonary perfusion (due to regional alveolar hypoxia) reduced the amount of measurable ACE circulating in the lungs. From this data the authors concluded that the technique was suitable to investigate in vivo expression of ACE.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

Hwang et al. (12) reported the use of [^18^F]FCAP in a normal male volunteer. The individual was injected with 7 mCi of the tracer and imaged sequentially at the lung and kidney levels five times using PET. After 90 min, the subject was given cold captopril orally, and 66 min later two more sequential images were taken at both levels. The lung/kidney ratio decreased from ~1.6 to 0.8 over the 90-min period before unlabeled captopril was administered. In contrast, for rats this ratio increased from ~5.3 to 7.9 over a 90-min period post-injection. On a weight/weight ratio basis, the human and the animals showed a similar uptake. In the human, the lungs showed an uptake 4.8 times that of the kidneys. However, the clearance rate from the lung in the human was higher than in the rats, whereas the opposite was observed with the kidneys. From these observations the authors concluded that results obtained with animals may not necessarily reflect the exact effect of a drug at the site of action in humans. According to these investigators, [^18^F]FCAP would be an excellent tool to study ACE dynamics in humans.

It was reported that inhibition of ACE delayed the onset of pulmonary hypertension (PPH) in animals due to pulmonary vascular remodeling (19). To determine if this was also true for humans, a study on the binding and inhibition of pulmonary ACE in humans using [^18^F]FCAP was initiated (20). For this study, the combined forward rate constant (CFRC) for pulmonary ACE in humans was determined. The CFRC is a product of the association constant (k_a_) and concentration of the ACE binding sites (B_max_); it is therefore proportional to the mass of ACE in the lungs. The CFRC decreased by 84% in five normal humans after they ingested 5 mg enalapril (an ACE inhibitor) daily for a week. In five patients with PPH who were given the same treatment, a decrease of 76% was observed in the CFRC. The investigators observed that individuals with PPH had a significantly reduced total mass of pulmonary ACE, and a low dose of an ACE inhibitor can delay vascular remodeling in such patients.

## References

1 Campbell DJ. (1987). Circulating and tissue angiotensin systems. J Clin Invest.
2 Chandrashekhar Y, Narula J. (2007). Exposing ACE up the sleeve. J Nuclear Med.
3 Dilsizian V, Eckelman WC, Loredo ML, Jagoda EM, Shirani J. (2007). Evidence for tissue angiotensin-converting enzyme in explanted hearts of ischemic cardiomyopathy using targeted radiotracer technique. J Nuclear Med.
4 Ondetti MA, Cushman DW. (1981). Inhibition of the renin-angiotensin system. A new approach to the therapy of hypertension. J Med Chem.
5 Kuoppala A, Lindstedt KA, Saarinen J, Kovanen PT, Kokkonen JO. (2000). Inactivation of bradykinin by angiotensin-converting enzyme and by carboxypeptidase N in human plasma. Am J Physiol Heart Circ Physiol.
6 Bohm K Kilter H Kindermann M Mechanisms contributing to the progression of left ventricular dysfunction to end-stage heart failure Eur Heart J Suppl 2003 5Suppl 114 21
7 Hirsch AT, Talsness CE, Schunkert H, Paul M, Dzau VJ. (1991). Tissue-specific activation of cardiac angiotensin converting enzyme in experimental heart failure. Circ res.
8 Paul M, Poyan Mehr A, Kreutz R. (2006). Physiology of local renin-angiotensin systems. Physiol Rev.
9 Shirani J, Dilsizian V. (2007). Molecular imaging of heart failure. Curr Opinion Biotechnol.
10 Shirani J, Narula J, Eckelman WC, Dilsizian V. (2006). Novel imaging strategies for predicting remodeling and evolution of heart failure:targeting the renin-angiotensin system. Heart Failure Clin.
11 Brunner-La Rocca HP, Vaddadi G, Esler MD. (1999). Recent insight into congestive heart failure:focus on ACE inhibition and angiotensin-II antagonism. J Am Coll Cardiol.
12 Hwang DR, Eckelman WC, Mathias CJ, Petrillo EW, Lloyd J, Welch MJ. (1991). Positron-labeled angiotensin-converting enzyme (ACE) inhibitor: fluorine-18-fluorocaptopril. Probing the ACE activity in vivo by positron emission tomography. J Nucl Med.
13 Strittmatter SM, Kapiloff MS, Snyder SH. (1983). [3H]Captopril binding to membrane associated angiotensin converting enzyme. Biochem Biophys Res Commun.
14 Heald AF, Ita CE, Singhvi SM, Migdalof BH. (1985). Tissue distribution of 14C- and 35S-captopril in rats after intravenous and oral administration. Xenobiotica.
15 Ikeda T, Komai T, Kawai K, Shindo H. (1981). Urinary metabolites of 1-(3-mercapto-2-D-methyl-oxopropyl)-L-proline (SQ14225), a new antihypertensive agent in rats and dogs. Chem Pharm Bull.
16 Wilson SK, Lynch DR, Snyder SH. (1987). Angiotensin-converting enzyme labeled with [3H]captopril. Tissue localizations and changes in different models of hypertension in the rat. J Clin Invest.
17 Markham J, McCarthy TJ, Welch MJ, Schuster DP. (1995). In vivo measurements of pulmonary angiotensin-converting enzyme kinetics. I. Theory and error analysis. J Appl Physiol.
18 Schuster DP, McCarthy TJ, Welch MJ, Holmberg S, Sandiford P, Markham J. (1995). In vivo measurements of pulmonary angiotensin-converting enzyme kinetics. II. Implementation and application. J Appl Physiol.
19 Nong Z, Stassen JM, Moons L, Collen D, Janssens S. (1996). Inhibition of tissue angiotensin-converting enzyme with quinapril reduces hypoxic pulmonary hypertension and pulmonary vascular remodeling. Circulation.
20 Qing F, McCarthy TJ, Markham J, Schuster DP. (2000). Pulmonary angiotensin-converting enzyme (ACE) binding and inhibition in humans. A positron emission tomography study. Am J Respir Crit Care Med.